# BM3h-8C8 Mutant of the heme domain of the bacterial cytochrome P450-BM3 (Bacillus megaterium)

Chemical name: | BM3h-8C8 Mutant of the heme domain of the bacterial cytochrome P450-BM3 (Bacillus megaterium)
Abbreviated name: | BM3h-8C8
Synonym:
Agent Category: | Proteins
Target: | Dopamine
Target Category: | Others (neurotransmitter)
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal / contrast: | Fe
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=molecular+imaging+and+dopamine+and+measurement)]

BM3h-8C8 is a mutant of the heme domain of the bacterial cytochrome P450-BM3 (BM3h) from Bacillus megaterium, and it was generated by Shapiro et al. with directed evolution of BM3h for magnetic resonance imaging (MRI) of dopamine (1).

Dopamine is a catecholamine neurotransmitter produced mainly by the medulla of the adrenal glands and the nervous tissues, including the substantia nigra and the ventral tegmental area (2, 3). In neurons, synthetic dopamine is packaged into vesicles and then released into the synapse in response to presynaptic action potentials. Dopamine also acts as a neurohormone, inhibiting prolactin release from the pituitary gland (4). Dopamine is of further significance because of its roles in learning, reward, and motor coordination, and because of the dysfunction of dopaminergic systems underlying addiction and neurodegenerative diseases (5-8). Radionuclides have been investigated for imaging dopamine and its receptors in vivo, but both positron emission tomography and single-photon emission tomography have low spatial and temporal resolution in spite of high sensitivity (9-12).

Shapiro et al. developed a dopamine sensor for MRI using directed evolution of BM3h (1). BM3h, a 53-kDa moiety, contains a single iron(III) atom bound to a hemin prosthetic group (13). The iron ion is the site of oxygen binding; when oxygen is not bound, a water molecule fills the site with a weak bond. Interaction of the heme iron with exchanging water molecules at this axial site could promote T_1_ relaxation and thus modulate MRI contrast (1). Studies by Shapiro et al. revealed an r_1_ value (T_1_ relaxivity; 1/T1) of 1.23 ± 0.07 mM−^1^s−^1^ for BM3h in phosphate-buffered saline without ligands. Addition of a saturating quantity of arachidonic acid, a natural BM3h substrate, resulted in an r_1_ value of 0.42 ± 0.05 mM−^1^s−^1^. This ligand-induced decrease in relaxivity, arising from the displacement of water molecules at the BM3h heme, enabled quantitative sensing of arachidonic acid with MRI. Further studies by Shapiro et al. showed that addition of 1 mM dopamine to BM3h induced a decrease in the r_1_ value to 0.76 ± 0.03 mM−^1^s−^1^, indicating that dopamine directly replaces water as an axial metal ligand in the BM3h substrate-binding pocket. The apparent dissociation constant (K_d_) for arachidonic acid was 6.8 ± 0.5 μM, and the K_d_ for dopamine was 990 ± 110 μM. These results suggest that BM3h could serve as a platform for molecular sensor engineering (1, 14, 15). Using the platform of BM3h, Shapiro et al. generated a series of MRI sensors for dopamine by decreasing the affinity for arachidonic acid, increasing the affinity for dopamine, and enhancing the relaxivity changes upon ligand binding with the directed evolution technique (1). Directed evolution is a molecular engineering method that utilizes successive rounds of mutagenesis and selection to generate proteins with novel functionality, starting from a molecule with some of the desired properties of the end product (14, 15). BM3h-8C8 is one of the BM3h-based mutants with the best combination of relaxivity change, improved affinity for dopamine, and decreased affinity for arachidonic acid (1).

### Related Resource Links:

- Chapters for dopamine and dopamine receptor imaging on MICAD (http://www.ncbi.nlm.nih.gov/books/?term=dopamine%20AND%20micad%5bbook%5d)
- Bioassays for dopamine and dopamine receptors in PubChem BioAssay (http://www.ncbi.nlm.nih.gov/pcassay/?term=dopamine,+dopamine+receptor)
- Dopamine-related articles in Online Mendelian Inheritance in Man (OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=dopamine))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20190737)]

Shapiro et al. generated BM3h-8C8 using directed evolution of BM3h (1). The wild-type (WT) BM3h with a C-terminal hexahistidine tag was housed in the pCWori vector. Mutant libraries were then produced through error-prone polymerase chain reaction (PCR) with the 5'-GAAACAGGATCCATCGATGCTTAGGAGGTCAT-3' (forward) and 5'-GCTCATGTTTGACAGCTTATCATCG-3' (reverse) primers. Input to each round of screening consisted of a library of BM3h mutants, each with an average of one to two amino acid substitutions, generated from the WT gene or a previously selected mutant. From each screen, eight to ten mutants were selected to determine their affinities for dopamine and arachidonic acid and to ensure the robustness of the ligand-induced changes in r_1_. Between the fourth and fifth rounds of evolution, the mutation I366V was introduced via overlap extension PCR to improve protein thermostability.

The BM3h-8C8 mutant had an optically determined K_d_ values of 8.9 ± 0.7 μM for dopamine and 750 ± 140 μM for arachidonic acid. The r_1_ values were 1.1 ± 0.1 mM−^1^s−^1^ in the absence of ligand and 0.17 ± 0.03 mM−^1^s−^1^ in the presence of 400 μM dopamine. BM3h-8C8 exhibited a dopamine concentration–dependent decrease in T_1_-weighted MRI signal (up to 13% with 28.5 μM protein) with an estimated K_d_ value of 4.9 ± 2.7 μM. Specificity analysis with MRI showed that only dopamine, norepinephrine, and serotonin elicited substantial changes in the T_1_ relaxation rate (1/T_1_) from the potential ligands of norepinephrine, 3,4-dihydroxy-L-phenylalanine, serotonin, glutamate, glycine, γ-aminobutyric acid, acetylcholine, and arachidonic acid. The 1/T_1_ reductions produced by norepinephrine and serotonin were 0.0076 ± 0.0023 s−^1^ and 0.0041 ± 0.0020 s−^1^, respectively, compared with 0.0182 ± 0.0006 s−^1^ for dopamine. The measured K_d_ values were 44 ± 3 μM and 80 ± 8 μM for norepinephrine and serotonin, respectively. Only monoamines had affinity for BM3h-8C8, whereas two catechols, epinephrine and 3,4-dihydrophenylacetic acid, both of which lack primary amines, showed no measurable affinity (data not shown). The primary amine in dopamine may serve as an axial ligand to the BM3h heme in the sensor-analyte complexes. BM3h-8C8 is specific for sensing dopamine at concentrations above 10 μM.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20190737)]

Shapiro et al. tested the ability of BM3h-8C8 to measure dopamine discharge from PC12 cells stimulated with extracellular K^+^ (54 mM) (1). K^+^ is a depolarizing stimulus to release dopamine, and K^+^ itself has no effect on r_1_ of the BM3h-8C8 (data not shown). PC12 is a cell line derived from a pheochromocytoma of the rat adrenal medulla and is useful as a cellular model of dopaminergic function. T_1_-Weighted MRI images (spin echo TE/TR = 10/477 ms) showed that BM3h-8C8 had a 37 ± 2% reduction in r_1_ in the supernatant of K^+^-stimulated cells relative to Na^+^ controls.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20190737)]

Shapiro et al. tested the ability of BM3h-8C8 to measure dopamine concentrations in intact rats (n = 5-7/group) (1). T_1_-Weighted MRI scans were performed continuously during paired infusions of BM3h-8C8 or control WT BM3h with and without dopamine via cannulae into the left and right striatum. Dopamine-dependent contrast changes were apparent in images obtained during and after infusion periods. Consistent with results obtained in vitro, addition of dopamine dampened the intensity enhancement by ~50% in the striatal regions of interest (P = 0.003). WT BM3h, which has a very low affinity for dopamine (K_d_ = ~1 mM), did not change the MRI intensity regardless of the presence or absence of dopamine (P = 0.8). Infusion of dopamine alone also produced no noticeable signal changes in an equivalent experiment (data not shown). These results indicate that the dopamine-dependent signal differences require the presence of a micromolar-affinity dopamine sensor and are not explained by physiological or biochemical effects of dopamine itself. On the basis of the relaxivity values measured for BM3h-8C8 in vitro, the estimated maximal concentrations were 89 ± 19 μM for BM3h-8C8 and 75 ± 28 μM for dopamine across the striatal regions. Histological analysis showed minimal evidence of toxicity due to these procedures.

Shapiro et al. then tested the ability of BM3h-8C8 to detect the release of endogenous dopamine in the rat brain (n = 6) (1). MRI data were acquired during co-infusion of BM3h-8C8 with elevated concentrations of K^+^. As the control, WT BM3h with K^+^ was infused into the opposite hemisphere. As additional controls, MRI signal changes in response to K^+^ stimulation and to dopamine were also studied in the absence of BM3h-8C8. MRI signal decreased significantly in response to K^+^ stimulation (P < 0.01), and the decrease was dopamine sensor–dependent. A discernable signal decrease of up to 3% was produced during each K^+^ stimulation period. The first K^+^ block evoked the largest response (presumably because of partial dopamine depletion over subsequent blocks) and elicited a clear spatiotemporal pattern of MRI signal change from baseline over the course of the stimulation period. The signal difference between low- and high-K^+^ stimulation was also significant (0.07%, P = 0.0008) for BM3h-8C8, but not for the control (−0.02%, P > 0.05). The results were consistent with the expected suppression of MRI signal by dopamine release under high-K^+^ conditions.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Shapiro M.G., Westmeyer G.G., Romero P.A., Szablowski J.O., Kuster B., Shah A., Otey C.R., Langer R., Arnold F.H., Jasanoff A. (2010). Directed evolution of a magnetic resonance imaging contrast agent for noninvasive imaging of dopamine. Nat Biotechnol.
2 Missale C., Nash S.R., Robinson S.W., Jaber M., Caron M.G. (1998). Dopamine receptors: from structure to function. Physiol Rev.
3 Nitsche M.A., Monte-Silva K., Kuo M.F., Paulus W. (2010). Dopaminergic impact on cortical excitability in humans. Rev Neurosci.
4 Samson W.K., Taylor M.M., Baker J.R. (2003). Prolactin-releasing peptides. Regul Pept.
5 Rogers R.D. (2011). The roles of dopamine and serotonin in decision making: evidence from pharmacological experiments in humans. Neuropsychopharmacology.
6 Arias-Carrion O., Stamelou M., Murillo-Rodriguez E., Menendez-Gonzalez M., Poppel E. (2010). Dopaminergic reward system: a short integrative review. Int Arch Med.
7 Bromberg-Martin E.S., Matsumoto M., Hikosaka O. (2010). Dopamine in motivational control: rewarding, aversive, and alerting. Neuron.
8 Gardian G., Vecsei L. (2010). Medical treatment of Parkinson's disease: today and the future. Int J Clin Pharmacol Ther.
9 Tatsch K. (2010). Positron emission tomography in diagnosis and differential diagnosis of Parkinson's disease. Neurodegener Dis.
10 Isaias I.U., Antonini A. (2010). Single-photon emission computed tomography in diagnosis and differential diagnosis of Parkinson's disease. Neurodegener Dis.
11 Van Laere K., Varrone A., Booij J., Vander Borght T., Nobili F., Kapucu O.L., Walker Z., Nagren K., Tatsch K., Darcourt J. (2010). EANM procedure guidelines for brain neurotransmission SPECT/PET using dopamine D2 receptor ligands, version 2. Eur J Nucl Med Mol Imaging.
12 Varrone A., Halldin C. (2010). Molecular imaging of the dopamine transporter. J Nucl Med.
13 Girvan H.M., Toogood H.S., Littleford R.E., Seward H.E., Smith W.E., Ekanem I.S., Leys D., Cheesman M.R., Munro A.W. (2009). Novel haem co-ordination variants of flavocytochrome P450BM3. Biochem J.
14 Glieder A., Farinas E.T., Arnold F.H. (2002). Laboratory evolution of a soluble, self-sufficient, highly active alkane hydroxylase. Nat Biotechnol.
15 Li Q.S., Schwaneberg U., Fischer P., Schmid R.D. (2000). Directed evolution of the fatty-acid hydroxylase P450 BM-3 into an indole-hydroxylating catalyst. Chemistry.